# 1-(1-Phenylethyl)-1H-imidazole-5-carboxylic acid [11C]methyl ester

Chemical name: | 1-(1-Phenylethyl)-1H-imidazole-5-carboxylic acid [^11^C]methyl ester
Abbreviated name: | [^11^C]MTO
Synonym: | [^11^C]Metomidate, [O-Methyl-^11^C]Metomidate
Agent category: | Compound
Target: | 11β-Hydroxylase
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20AND%20metomidate)]

In the adrenocortex, 11β-hydroxylase is a key enzyme in the biosynthesis of cortisol and aldosterone. This enzyme can be overexpressed in adrenocortical carcinomas, which secrete excessive amounts of catecholamines and cortical hormone (1). However, some adrenal tumors appear unexpectedly as incidentalomas in computed tomography (CT), magnetic resonance imaging (MRI) and ultrasound scans in 1-4% of patients (2). Most of these incidentalomas consist of benign, cortical, nonhypersecretory adenomas (3). Therefore, it is important to identify the malignant lesions in the incidentalomas for appropriate clinical treatments. Ketoconazole, etomidate and metomidate are potent inhibitors of 11β-hydroxylase (4, 5). [^11^C]Metomidate introduced as an adrenocortical imaging tracer by Bergstrom et al. (6) has proven to be useful in distinguishing adrenocortical from non-cortical lesions and identifying incidentalomas of adrenocortical origin (7-10).

### Related Resource Links:

- Chapters in MICAD (11β-Hydroxylase (http://www.ncbi.nlm.nih.gov/books?term=11%CE%B2-hydroxylase%20%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (11β-Hydroxylase (http://www.ncbi.nlm.nih.gov/gene/90299))
- Articles in Online Mendelian Inheritance in Man (OMIM) (11β-Hydroxylase (http://omim.org/entry/202010))
- Clinical trials ([^11^C]Metomidate (http://www.clinicaltrials.gov/ct2/results?term=Metomidate&Search=Search))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(11C%20AND%20metomidate)%20and%20synthesis)]

[^11^C]MTO was first synthesized by reacting (R)-1-(1-phenylethyl)-1H-imidazole-5-carboxylic acid with [^11^C]methyl iodide with low recovery yields by preparative high-performance liquid chromatography (HPLC) (6). The specific activity was up to 120 GBq/μmol (3.2 Ci/μmol). Later, [^11^C]MTO was purified with an improved preparative HPLC method to >99% radiochemical purity (11). The overall yield was 19.9% (not decay corrected, based on [^11^C]methyl iodide) in 34 min. The specific activity was up to 63.3 GBq/μmol (1.71 Ci/μmol) averaging 14.4 GBq/μmol (0.389 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(11C%20AND%20metomidate)%20and%20in%20vitro)]

In vitro frozen section autoradiography with [^11^C]MTO in different tissues from rats and pigs were measured (6). The adrenals have the highest uptake, followed by the livers (26% of adrenal uptake). The uptake by pig adrenal slices linearly increased with time. A plateau was seen at about 40-50 min. The nonspecific binding was 2% for [^11^C]MTO and 13% for [^11^C]etomidate. [^11^C]MTO (30 nM) binding to pig adrenal cortex was inhibited by etomidate with an IC_50_ of 0.4 μM. Etomidate inhibited the [^11^C]MTO binding to liver slices with an IC_50_ of 0.07 μM. There was a clear correlation of 11β-hydroxylase staining to [^11^C]MTO binding in different tissue slices. Human adenomas showed strong 11β-hydroxylase staining and high [^11^C]MTO binding (1.40 ± 0.76) as compared with nonadrenal cancers with weak staining and low binding (0.17 ± 0.15).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(11C%20AND%20metomidate)%20and%20rodentia)]

No relevant publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(11C%20and%20metomidate)%20and%20(dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep))]

No relevant publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(11C%20and%20metomidate)%20and%20primate%20not%20human)]

Positron emission tomography (PET) studies in three rhesus monkeys showed high uptake of [^11^C]MTO in the adrenals with excellent visualization (6). The uptake increased with time without washout at 45 min after injection. Slightly lower uptake was seen in the liver as compared with the adrenals. No other organs besides the adrenals and livers have any uptake at 45 min.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20-metomidate%20and%20human)]

[^11^C]MTO PET was performed in 15 patients with unilateral adrenal lesions as confirmed by CT (12). [^11^C]MTO (294-938 MBq, 8-25 mCi) was intravenously injected into patients. All cortical lesions were easily visualized with high tracer uptake, whereas the noncortical lesions showed very low uptake at 5 to 40 min after injection. High uptake was seen in the stomach, normal adrenals, and liver. The kidney and spleen reached a moderate uptake within a few min after injection and then declined rapidly to almost background levels.

[^11^C]MTO PET studies were performed in 11 patients with CT-detected primary tumors or recurrence and/or metastases from a previously histopathologically proven adrenocortical carcinoma The PET findings were compared with the CT scan findings and verified by histopathology. Primary adrenocortical carcinoma showed increased [^11^C]MTO uptake compared with normal adrenal, liver, and other normal tissues (such as the spleen, kidney, and muscle). The high liver metastasis to normal liver background ratio contributed to the better sensitivity of tumor detection by PET. When all visible lesions were considered, uptake (SUV, 16.4 ± 2.2) was higher than in adrenals (SUV, 11.5 ± 1.5; p < 0.02), liver (SUV, 8.9 ± 0.9; p < 0.005), spleen, kidney, and muscle (all, p < 0.001). Normal adrenal had higher uptake than liver (p < 0.02) and all other normal tissues (p < 0.001), whereas liver showed higher uptake than all other normal organs except adrenal (p < 0.0001). It was noted that chemotherapy and treatment with adrenal steroid inhibitors decreased [^11^C]MTO uptake and may interfere with lesion detection.

[^11^C]MTO PET studies were performed recently in 21 patients with adrenal incidentalomas (9) and in 16 patients with adrenocortical lesions (10). Both studies concluded that [^11^C]MTO uptake was able to distinguish between adrenocortical and nonadrenocortical lesions. FDG was found to be a better PET tracer than [^11^C]MTO in distinguishing between benign and malignant adrenal lesions. Internal dosimetry data for [^11^C]MTO in humans is not available in the literature.

## References

1 Suzuki H., Shibata H., Maruyama T., Ishimura Y., Saruta T. (1995). Significance of steroidogenic enzymes in the pathogenesis of hyperfunctioning and non-hyperfunctioning adrenal tumor. Steroids.
2 Bertherat J., Mosnier-Pudar H., Bertagna X. (2002). Adrenal incidentalomas. Curr Opin Oncol.
3 Kloos R.T., Gross M.D., Francis I.R., Korobkin M., Shapiro B. (1995). Incidentally discovered adrenal masses. Endocr Rev.
4 Engelhardt D. (1994). Steroid biosynthesis inhibitors in Cushing's syndrome. Clin Investig.
5 Varga I., Racz K., Kiss R., Futo L., Toth M., Sergev O., Glaz E. (1993). Direct inhibitory effect of etomidate on corticosteroid secretion in human pathologic adrenocortical cells. Steroids.
6 Bergstrom M., Bonasera T.A., Lu L., Bergstrom E., Backlin C., Juhlin C., Langstrom B. (1998). In vitro and in vivo primate evaluation of carbon-11-etomidate and carbon-11-metomidate as potential tracers for PET imaging of the adrenal cortex and its tumors. J Nucl Med.
7 Bergstrom M., Sorensen J., Kahn T.S., Juhlin C., Eriksson B., Sundin A., Bonasera T.A., Fasth K., Langstrom B. (1999). PET with [11C]-Metomidate for the Visualization of Adrenocortical Tumors and Discrimination from Other Lesions. Clin Positron Imaging.
8 Khan T.S., Sundin A., Juhlin C., Langstrom B., Bergstrom M., Eriksson B. (2003). 11C-metomidate PET imaging of adrenocortical cancer. Eur J Nucl Med Mol Imaging.
9 Minn H., Salonen A., Friberg J., Roivainen A., Viljanen T., Langsjo J., Salmi J., Valimaki M., Nagren K., Nuutila P. (2004). Imaging of adrenal incidentalomas with PET using (11)C-metomidate and (18)F-FDG. J Nucl Med.
10 Zettinig G., Mitterhauser M., Wadsak W., Becherer A., Pirich C., Vierhapper H., Niederle B., Dudczak R., Kletter K. (2004). Positron emission tomography imaging of adrenal masses: (18)F-fluorodeoxyglucose and the 11beta-hydroxylase tracer (11)C-metomidate. Eur J Nucl Med Mol Imaging.
11 Mitterhauser M., Wadsak W., Langer O., Schmaljohann J., Zettinig G., Dudczak R., Viernstein H., Kletter K. (2003). Comparison of three different purification methods for the routine preparation of [11C] Metomidate. Appl Radiat Isot.
12 Bergstrom M., Juhlin C., Bonasera T.A., Sundin A., Rastad J., Akerstrom G., Langstrom B. (2000). PET imaging of adrenal cortical tumors with the 11beta-hydroxylase tracer 11C-metomidate. J Nucl Med.